# (R)-2-[^11^C]Methoxy-N-n-propylnorapomorphine

Chemical name: | (R)-2-[^11^C]Methoxy-N-n-propylnorapomorphine
Abbreviated name: | [^11^C]MNPA
Synonym:
Agent Category: | Compound
Target: | Dopamine receptors (D_2_ and D_3_)
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20MNPA)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion (1, 2). Dopamine receptors are involved in the pathophysiology of neuropsychiatric diseases, such as Parkinson’s disease, Alzheimer's disease, Huntington’s disease, and schizophrenia (3). Five subtypes of dopamine receptors, D_1_ through D_5_, have been well characterized pharmacologically and biochemically (4). These five subtypes are classified into two subfamilies: D_1_-like (D_1_ and D_5_) and D_2_-like (D_2_, D_3_, and D_4_) dopamine receptors. D_1_- and D_2_-like receptors exert synergistic as well as opposite effects at both the biochemical and overall system level. A great majority of striatal D_1_ and D_2_ receptors are localized postsynaptically on caudate-putamen neurons and to a lesser extent presynaptically on nigrostriatal axons.

Dopamine receptors are G-protein-coupled receptors and exist in high- and low-affinity states with respect to agonist binding. The two states are interconvertible. In the high-affinity state, the receptor is coupled to G-proteins, whereas in the low-affinity state, it is not. Dopamine has a K_d_ of 7 nM for the high-affinity state (K_high_) and a K_d_ of 1,720 nM for the low-affinity state (K_low_) (5). Under physiologic conditions, dopamine is expected to bind predominately to receptors in the high-affinity state. The high-affinity state has been suggested to be the functional form of the dopamine receptors.

Substituted benzamides, such as sulpiride, raclopride, and iodobenzamide, are specific ligands with only moderate affinity for the D_2_ receptors, making studies of extrastriatal D_2_ receptors difficult (6-8). In binding studies, [^123^I]-labeled epidepride, an analog of isoremoxipride, was found to have high potency and low nonspecific binding and to be selective for striatal and extrastriatal D_2_ receptors (9). Epidepride has marginal binding to D_4_ receptors, with little affinity for other known neurotransmitter receptors. (S)-N-((1-Allyl-2-pyrrolidinyl)methyl)-5-(3-[^18^F]fluoropropyl)-2,3-dimethoxybenzamide ([^18^F]fallypride), an analog of epidepride, was found to be a selective, high-affinity antagonist of D_2/3_ receptors (10), and in positron emission tomography (PET) in vivo studies (11-13), it identified extrastriatal D_2/3_ receptors. However, none of these antagonists distinguishes between the high- and low-affinity states of the D_2_ receptors. (–)-N-Propyl-norapomorphine (NPA) was reported to have K_high_ and K_low_ values of 0.07-0.4 and 20-200 nM, respectively (5, 14-16). This provides a >50-fold selectivity for the high-affinity over the low-affinity receptors. NPA has good affinity (K_i_ = 0.3 nM) for D_3_ receptors but not for other neurotransmitters (17). (R)-2-Methoxy-N-n-propylnorapomorphine (MNPA) is a methoxy analog of NPA and a selective D_2_-like receptor agonist with a high affinity (K_i_ = 0.17 nM) and a D_2_/D_1_ potency ratio of 10,500 (18, 19). [^11^C]MNPA is being developed as a PET agent for the non-invasive study of the high-affinity state of the D_2/3_ receptors in the brain.

.

### Related Resource Links:

- Chapters in MICAD (Dopamine receptors (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=dopamine%20(receptors%20OR%20receptor)+%20AND+Table+AND+micad%5Bbook%5D))
- Gene information in NCBI (D_2_ receptor, (http://www.ncbi.nlm.nih.gov/gene/1813) D_3_ receptor (http://www.ncbi.nlm.nih.gov/gene/1814))
- Articles in Online Mendelian Inheritance in Man (OMIM) (D_2_ receptor (http://www.ncbi.nlm.nih.gov/omim/126450), D_3_ receptor (http://www.ncbi.nlm.nih.gov/omim/126451))
- Clinical trials (Dopamine receptors (http://www.clinicaltrials.gov/ct2/results?term=dopamine+receptor))
- Drug information in Food and Drug Administration (Dopamine receptors (http://google2.fda.gov/search?q=dopamine+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=6&y=12))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20MNPA%20and%20synthesis)]

Finnema et al. (20) reported a synthesis of [^11^C]MNPA that involved direct O-methylation of (R)-2-hydroxy-NPA with [^11^C]methyl iodide and NaOH in dimethyl sulfoxide, with a radiochemical yield of 75% (based on [^11^C]methyl iodide) at end of synthesis and an average specific activity of 13 GBq/μmol (350 Ci/mmol at end of synthesis) after high-performance liquid chromatography (HPLC) purification. Radiochemical purities were >98% with a total synthesis time of 30-35 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20MNPA%20and%20in%20vitro)]

In competition binding to dopamine receptors in membranes of rat striatum, MNPA had K_i_ values of 1,780 and 0.17 nM for D_1_ and D_2_ receptors, respectively. The D_2_/D_1_ potency ratio was 10,500 for MNPA (19).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%20and%20MNPA%29%20and%20rodentia)]

Seneca et al. (21) performed [^11^C]MNPA PET brain scans in normal male rats for 90 min. The striatal binding potential (BP_ND_) values (n = 5) were 0.93 ± 0.12 and 0.83 ± 0.13 for kinetic and equilibrium reference tissue (cerebellum) methods, respectively. Depletion of endogenous dopamine with reserpine plus α-methyl-p-tyrosine increased the BP_ND_ values by ~100%. Thus, occupancy by D2/3 receptors by endogenous dopamine was calculated to be ~53%. Raclopride (2 mg/kg) displaced striatal activity by ~83% when injected during the steady state (50 min after injection of [^11^C]MNPA), whereas BP 897 (a selective D_3_ compound, 0.5 mg/kg) displaced the striatal activity by <10%. There were two less lipophilic radiometabolites and one more lipophilic radiometabolite than MNPA with 10% of total radioactivity in the brain at 30 min after injection. On the other hand, there was 8% of radiometabolites in the brain after dopamine depletion. Radiometabolites in the plasma were 71.4 ± 16.4% of total radioactivity at baseline and 61.3 ± 19.3% after dopamine depletion.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%20and%20MNPA%29%20and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%20and%20MNPA%29%20and%20%28primate%20not%20human%29)]

[^11^C]MNPA PET studies in non-human primates have provided useful assessment of the D_2_ receptor in the brain, showing localization of [^11^C]MNPA in the putamen and caudate. Finnema et al. (20) showed highest uptake in the striatum, moderate uptake in the thalamus, and low uptake in the cerebellum of 2 cynomolgus monkeys, with a striatum/cerebellum ratio of 2.23 ± 0.21 and thalamus/cerebellum ratio of 1.37 ± 0.06 at 72-78 min after injection of 56 MBq (1.5 mCi) of [^11^C]MNPA. About 4.5% of the injected radioactivity was in the brain at 5 min. This uptake is higher than the 1-2% reported previously for [^11^C]raclopride, a D_2_ antagonist (22). The striatal accumulation of [^11^C]MNPA was inhibited (79% reduction) by pretreatment with raclopride (1 mg/kg) with a striatum/cerebellum ratio of 1.26 at 78 min after injection. The fraction of unchanged [^11^C]MNPA in plasma, as determined by HPLC, was 50 and 20% at 4 and 45 min after injection, respectively. All radiolabeled metabolites were more polar than the parent compound and would not be expected to cross the blood-brain barrier.

Seneca et al. (23) studied 4 cynomolgus monkeys with [^11^C]raclopride (a D_2_ antagonist) and [^11^C]MNPA under baseline conditions and after administration of the potent dopamine releaser amphetamine. A two-parameter multilinear reference tissue model was used to derive the striatal binding potential (BP). The [^11^C]raclopride BP was reduced by 2, 16, 15, and 23% after amphetamine doses of 0.1, 0.2, 0.5, and 1.0 mg/kg, respectively. [^11^C]MNPA BP was reduced by 4, 23, 25, and 46% after amphetamine doses of 0.1, 0.2, 0.5, and 1.0 mg/kg, respectively. Thus, endogenous dopamine was 50% more effective at competing with [^11^C]MNPA binding compared with [^11^C]raclopride binding, which is consistent with the pharmacology of these tracers (agonist versus antagonist). These results also suggest that 61% of D_2_ receptors are configured in a state of high affinity for agonists in vivo. [^11^C]MNPA is able to detect the change in dopamine levels induced by D-amphetamine and is more vulnerable to competition by endogenous dopamine than by the antagonist radiotracer [^11^C]raclopride. The large proportion of high-affinity sites might explain the vulnerability of D_2_ radiotracers to competition by endogenous dopamine and is consistent with the reported in vivo binding of the agonist radiotracer [^11^C]MNPA. Raclopride would be expected to bind to both high- and low-affinity sites with the same affinity and therefore would be present in proportion to the ratio of the sites. Dopamine competes only at high-affinity sites; therefore, the competition with MNPA, which also is bound only to high-affinity sites, will be more efficient.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%20and%20MNPA%29%20and%20human)]

Otsuka et al. (24) performed 90-min dynamic PET scans in 10 healthy men (age = 27.7 ± 5.4 y) after an intravenous injection of 219 MBq (6 mCi) [^11^C]MNPA. BP_ND_ was calculated using the indirect kinetic method with a metabolite-corrected arterial input function, the simplified reference tissue model (SRTM) and transient equilibrium methods. BP_ND_ values obtained by kinetic analysis were 0.82 ± 0.09, 0.59 ± 0.11, and 0.28 ±0.06 in the putamen, caudate, and thalamus, respectively. BP_ND_ values obtained by the SRTM and transient equilibrium methods were in good agreement with those obtained by the indirect kinetic method (r = 0.98 and r = 0.93, respectively).

## NIH Support

Intramural Research Program

## References

1 Carbon M., et al. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Seeman P., et al. (1987). Human brain D1 and D2 dopamine receptors in schizophrenia, Alzheimer's, Parkinson's, and Huntington's diseases. Neuropsychopharmacology.
4 Stoof J.C., Kebabian J.W. (1984). Two dopamine receptors: biochemistry, physiology and pharmacology. Life Sci.
5 George S.R., et al. (1985). The functional state of the dopamine receptor in the anterior pituitary is in the high affinity form. Endocrinology.
6 Gehlert D.R., Wamsley J.K. (1984). Autoradiographic localization of [3H]sulpiride binding sites in the rat brain. Eur J Pharmacol.
7 Lidow M.S., et al. (1989). Dopamine D2 receptors in the cerebral cortex: distribution and pharmacological characterization with [3H]raclopride. Proc Natl Acad Sci U S A.
8 Brucke T., et al. (1988). In vitro binding properties and autoradiographic imaging of 3-iodobenzamide ([125I]-IBZM): a potential imaging ligand for D-2 dopamine receptors in SPECT. Life Sci.
9 Kessler R.M., et al. (1991). High affinity dopamine D2 receptor radioligands. 2. [125I]epidepride, a potent and specific radioligand for the characterization of striatal and extrastriatal dopamine D2 receptors. Life Sci.
10 Mukherjee J., et al. (1995). Fluorinated benzamide neuroleptics--III. Development of (S)-N-[(1-allyl-2-pyrrolidinyl)methyl]-5-(3-[18F]fluoropropyl)-2, 3-dimethoxybenzamide as an improved dopamine D-2 receptor tracer. Nucl Med Biol.
11 Grunder G., et al. (2006). The striatal and extrastriatal d2/d3 receptor-binding profile of clozapine in patients with schizophrenia. Neuropsychopharmacology.
12 Mukherjee J., et al. (2005). Measurement of d-amphetamine-induced effects on the binding of dopamine D-2/D-3 receptor radioligand, 18F-fallypride in extrastriatal brain regions in non-human primates using PET. Brain Res.
13 Riccardi P., et al. (2006). Amphetamine-induced displacement of [(18)f] fallypride in striatum and extrastriatal regions in humans. Neuropsychopharmacology.
14 Gardner B., Strange P.G. (1998). Agonist action at D2(long) dopamine receptors: ligand binding and functional assays. Br J Pharmacol.
15 Lahti R.A., et al. (1996). Affinities and intrinsic activities of dopamine receptor agonists for the hD21 and hD4.4 receptors. Eur J Pharmacol.
16 Seeman P., et al. (1985). Dopamine D2 receptor binding sites for agonists. A tetrahedral model. Mol Pharmacol.
17 Neumeyer J.L., et al. (1973). Aporphines. 8. Total synthesis and pharmacological evaluation of (plus or minus)-apomorphine, (plus or minus)-apocodeine, (plus or minus)-N-n-propylnorapomorphine, and (plus or minus)-N-n-propylnorapocodeine. J Med Chem.
18 Gao Y.G., et al. (1990). Synthesis and dopamine receptor affinities of enantiomers of 2-substituted apomorphines and their N-n-propyl analogues. J Med Chem.
19 Neumeyer J.L., et al. (1990). Synthesis and dopamine receptor affinity of (R)-(-)-2-fluoro-N-n-propylnorapomorphine: a highly potent and selective dopamine D2 agonist. J Med Chem.
20 Finnema S.J., et al. (2005). A preliminary PET evaluation of the new dopamine D2 receptor agonist [11C]MNPA in cynomolgus monkey. Nucl Med Biol.
21 Seneca N., et al. (2008). Occupancy of dopamine D2/3 receptors in rat brain by endogenous dopamine measured with the agonist positron emission tomography radioligand [11C]MNPA. Synapse.
22 Farde L., et al. (1987). PET analysis of human dopamine receptor subtypes using 11C-SCH 23390 and 11C-raclopride. Psychopharmacology (Berl).
23 Seneca N., et al. (2006). Effect of amphetamine on dopamine D2 receptor binding in nonhuman primate brain: a comparison of the agonist radioligand [11C]MNPA and antagonist [11C]raclopride. Synapse.
24 Otsuka T., et al. (2009). Quantitative PET analysis of the dopamine D2 receptor agonist radioligand 11C-(R)-2-CH3O-N-n-propylnorapomorphine in the human brain. J Nucl Med.